# N-(2-(Diethylamino)ethyl)-5-[^123^I]iodonicotinamide

Chemical name: | N-(2-(Diethylamino)ethyl)-5-[^123^I]iodonicotinamide
Abbreviated name: | [^123^I]MEL008, [^123^]1
Synonym:
Agent category: | Compound
Target: | Melanins
Target category: | Receptor
Method of detection: | single photon emission computed tomography (SPECT)
Source of signal: | ^123^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iodonicotinamide)]

Malignant melanoma is the sixth most common cancer in the United States (1). Early diagnosis and prompt surgical removal comprise the best approach for a possible cure because malignant melanoma is a very aggressive cancer (2). Melanomas develop from activated or genetically altered neoplastic melanocytes that contain melanin (3-5). Melanin pigment is synthesized and deposited within melanosomes (6). Eumelanin and pheomelanin are the two major types of melanin. Eumelanin is the predominant melanin pigment found in primary tumors. Pheomelanin tends to associate with progression of the disease. Melanins are complex, negatively charged molecules with hydrophobic surfaces, and they have the capability to bind many different types of compounds (3). Therefore, melanins represent a very attractive target for both diagnosis and treatment.

Benzamide (BZA) derivatives and iodobenzamides have been found to have affinity for melanomas (3, 7-9). The exact mechanisms of uptake of these compounds have not been fully established (7, 10, 11). Direct melanin binding, involvement in the melanin biosynthesis pathway, and sigma (σ) receptor mediation have been proposed as the most likely mechanisms for different compounds. In addition, available vascular concentrations of these compounds and their ability to transport into the melanoma cells also influence their cellular uptake (11). Melanin-targeting radiopharmaceuticals that are based on BZA such as [^123^I]BZA, [^123^I]BZA_2_, and [^123^I]IBZM have been investigated and developed for molecular imaging of malignant melanomas (12-14). To produce a radioiodinated probe with higher tumor uptake and faster body clearance, Liu et al. (15) designed and prepared N-(2-(diethylamino)ethyl)-5-[^123^I]iodonicotinamide ([^123^I] MEL008), which has an alkylpiperazinyl moiety. Their study showed that [^123^I]MEL008 has a high selective uptake in the murine B16F0 melanoma tumor, and the uptake was most likely related to melanin binding and not to σ receptor binding.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Melanin+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (Melanin (http://www.ncbi.nlm.nih.gov/gene/5367))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=melanin)
- Information about N-(2-(diethylamino)ethyl)-5-[^123^I]iodonicotinamide ([^123^I] MEL008) in PubChem (http://www.ncbi.nlm.nih.gov/sites/entrez?cmd=search&db=pcsubstance&term=85756801)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iodonicotinamide%20and%20synthesis)]

Liu et al. (15) reported the synthesis of [^123^I]MEL008 by the standard peracetic acid oxidative radioiodination of the 5-trimethylstannyl derivative. [^123^I]MEL008 was purified with HPLC with a radiochemical purity of >95% and a specific activity of >2 GBq/nmol (54 mCi/nmol) at EOS. Lipophilicity of [^123^I]MEL008 was 1.55 (log P_7.5_) as determined by HPLC.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iodonicotinamide%20and%20in%20vitro)]

In vitro competitive binding assays of unlabeled MEL008 to σ_1_ and σ_2_ receptors in guinea pig brain membranes were conducted with 2 nM [^3^H](+)-pentazocine and 100 nM [^3^H]1,3-di-o-tolylguanidine, respectively. Very low affinities for both receptors were found. MEL008 exhibited K_i_ values of 3,100 and >50,000 nM for σ_1_ and σ_2_ receptors, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iodonicotinamide%20and%20rodentia)]

Liu et al. (15) performed biodistribution studies in black mice (n = 5/group) bearing murine melanotic B-16F0 or nude mice bearing A375 human amelanotic melanoma tumors after injection of 0.37-0.74 MBq (10-20 μCi) [^123^I]MEL008. In the B16F0 tumor model, there was high tumor radioactivity uptake, low normal organ radioactivity uptake, and rapid body clearance. The tumor radioactivity levels in percentage injected dose per gram (% ID/g) were 7.8 ± 1.7 (1 h), 6.0 ± 0.4 (3 h), 5.9 ± 0.7 (6 h), 3.2 ± 0.9 (24 h), and 2.2 ± 0.4 (48 h). At 1 h, the radioactivity levels (% ID/g) in other major organs were 2.0 ± 0.4 (liver), 1.8 ± 0.3 (kidney), 1.4 ± 0.2 (lung), 0.8 ± 0.1 (heart), 0.14 ± 0.02 (brain), and 1.2 ± 0.2 (blood). At 24 h, these levels (% ID/g) decreased to 0.12 (liver), 0.03 (kidney), 0.04 (lung), 0.15 (heart), 0.01 (brain), and 0.03 (blood). The tumor/mouse mean contrast ratios (MCR) were 4 (1 h), 7 (3 h), 12 (6 h), 37 (24 h), and 22 (48 h). The thyroid activity uptakes (% ID) were minimal, ranging from 0.37 ± 0.07 at 1 h to 1.4 ± 0.3 at 48 h. In comparison, a similar normal organ distribution pattern was observed in the A375 amelanotic melanoma, but the tumor radioactivity levels (n = 5) were very low with 0.40 ± 0.16% ID/g (1 h), 0.13 ± 0.06% ID/g (6 h), and 0.00I% D/g (24 h). The MCR values were 14 (1 h), 2 (6 h), and 0.04 (24 h). A blocking study was performed in the B16F0 mice with 1 mg/kg haloperidol (σ_1_ and σ_2_ inhibitor) administered 5 min before the [^123^I]MEL008 injection. At 1 h and 24 h, no inhibition was observed in the tumor, liver, kidney, and lung. Metabolic studies were performed by injecting 3–5 MBq (0.081–0.135 mCi) [^123^I]MEL008 into mice bearing B16F0 tumors. Plasma, brain, and tumor samples were obtained at 0.25, 1, and 24 h after injection. Thin-layer chromatography analysis indicated that 70-80% of the plasma radioactivity represented polar radioactive metabolites at 0.25-24 h. At these time points, 70-90% of the radioactivity in the brain and tumor represented intact [^123^I]MEL008. Gamma planar imaging was performed in mice bearing B16F0 melanotic tumors or A375 amelanotic melanomas. A dose of 10 MBq (0.27 mCi) [^123^I]MEL008 was administered by i.v. injection, and images were obtained 0.5 and 24 h after injection. The results showed that mice bearing B16F0 tumors and urinary bladder had the highest tumor radioactivity levels at 24 h. The eyes and thyroid were visualized with lower radioactivity levels. In comparison, only the urinary bladder and thyroid were visualized in the A375 tumor mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iodonicotinamide%20and%20(dog%20or%20pig%20or%20sheep%20or%20rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iodonicotinamide%20and%20(primate%20not%20human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iodonicotinamide%20and%20human)]

No publication is currently available.

## References

1 Miao Y., Benwell K., Quinn T.P. (2007). 99mTc- and 111In-labeled alpha-melanocyte-stimulating hormone peptides as imaging probes for primary and pulmonary metastatic melanoma detection. J Nucl Med.
2 Miao Y., Hylarides M., Fisher D.R., Shelton T., Moore H., Wester D.W., Fritzberg A.R., Winkelmann C.T., Hoffman T., Quinn T.P. (2005). Melanoma therapy via peptide-targeted {alpha}-radiation. Clin Cancer Res.
3 Dadachova E., Casadevall A. (2005). Melanin as a potential target for radionuclide therapy of metastatic melanoma. Future Oncol.
4 Cohen-Solal K.A., Crespo-Carbone S.M., Namkoong J., Mackason K.R., Roberts K.G., Reuhl K.R., Chen S. (2002). Progressive appearance of pigmentation in amelanotic melanoma lesions. Pigment Cell Res.
5 Sulaimon S.S., Kitchell B.E. (2003). The biology of melanocytes. Vet Dermatol.
6 Hearing V.J. (2000). The melanosome: the perfect model for cellular responses to the environment. Pigment Cell Res.
7 Pham, T.Q., P. Berghofer, X. Liu, I. Greguric, B. Dikic, P. Ballantyne, F. Mattner, V. Nguyen, C. Loc'h, and A. Katsifis, Preparation and Biologic Evaluation of a Novel Radioiodinated Benzylpiperazine, 123I-MEL037, for Malignant Melanoma. J Nucl Med, 2007
8 Michelot J.M., Moreau M.F., Veyre A.J., Bonafous J.F., Bacin F.J., Madelmont J.C., Bussiere F., Souteyrand P.A., Mauclaire L.P., Chossat F.M., et al. (1993). Phase II scintigraphic clinical trial of malignant melanoma and metastases with iodine-123-N-(2-diethylaminoethyl 4-iodobenzamide). J Nucl Med.
9 Wolf M., Bauder-Wust U., Mohammed A., Schonsiegel F., Mier W., Haberkorn U., Eisenhut M. (2004). Alkylating benzamides with melanoma cytotoxicity. Melanoma Res.
10 Dittmann H., Coenen H.H., Zolzer F., Dutschka K., Brandau W., Streffer C. (1999). In vitro studies on the cellular uptake of melanoma imaging aminoalkyl-iodobenzamide derivatives (ABA). Nucl Med Biol.
11 Eisenhut M., Hull W.E., Mohammed A., Mier W., Lay D., Just W., Gorgas K., Lehmann W.D., Haberkorn U. (2000). Radioiodinated N-(2-diethylaminoethyl)benzamide derivatives with high melanoma uptake: structure-affinity relationships, metabolic fate, and intracellular localization. J Med Chem.
12 Brandau W., Niehoff T., Pulawski P., Jonas M., Dutschka K., Sciuk J., Coenen H.H., Schober O. (1996). Structure distribution relationship of iodine-123-iodobenzamides as tracers for the detection of melanotic melanoma. J Nucl Med.
13 Moins N., D'Incan M., Bonafous J., Bacin F., Labarre P., Moreau M.F., Mestas D., Noirault E., Chossat F., Berthommier E., Papon J., Bayle M., Souteyrand P., Madelmont J.C., Veyre A. (2002). 123I-N-(2-diethylaminoethyl)-2-iodobenzamide: a potential imaging agent for cutaneous melanoma staging. Eur J Nucl Med Mol Imaging.
14 Salopek T.G., Scott J.R., Joshua A.V., Smylie M., Logus J.W., Morin C.A., McEwan A.J. (2001). Radioiodinated N-[3-(4-morpholino)propyl]-N-methyl-2-hydroxy-5-iodo-3-methylbenzylamine (ERC9): a new potential melanoma imaging agent. Eur J Nucl Med.
15 Liu X., Pham T.Q., Berghofer P., Chapman J., Greguric I., Mitchell P., Mattner F., Loc'h C., Katsifis A. (2008). Synthesis and evaluation of novel radioiodinated nicotinamides for malignant melanoma. Nucl Med Biol.